# 1-(4-[^18^F]Fluoroethoxy-3-methoxyphenethyl)-4-(3-phenylpropyl)piperazine

Chemical name: | 1-(4-[^18^F]Fluoroethoxy-3-methoxypheneσthyl)-4-(3-phenylpropyl)piperazine
Abbreviated name: | [^18^F]FE-SA4503
Synonym: | [^18^F]Fluoroethyl SA4503
Agent Category: | Compound
Target: | Sigma (σ) receptor
Target Category: | Receptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal/contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem.

## Background

[PubMed]

1-(4-[^18^F]Fluoroethoxy-3-methoxyphenethyl)-4-(3-phenylpropyl)piperazine ([^18^F]FE-SA4503) is a radioligand developed for positron emission tomography (PET) imaging of the sigma (σ) receptors. It is a potent sigma 1 (σ_1_) receptor agonist labeled with ^18^F, a positron emitter with a physical half-life (t_½_) of 109.8 min (1).

Sigma receptors are functional, membrane-bound proteins distributed in the central nervous system (CNS) and peripheral organs (2). The CNS sigma receptors are unique binding sites related to higher brain functions (3). They are distinct from opiate and phencyclidine (PCP) binding sites. There are at least two subtypes of sigma receptors, σ_1_ and σ_2_ receptors. The precise mechanism of the functional response of these receptors is not entirely known. These receptors appear to be involved in numerous pharmacological and physiological functions, and they also modulate a number of central neurotransmitter systems, including noradrenergic, glutamatergic, and dopaminergic systems. PCP and derivatives, cocaine and derivatives, some neuroleptics, atyptical antipsychotic agents, and other chemically unrelated compounds can bind to the sigma receptor sites. Studies have shown that these receptors may play a role in pathogenesis of psychiatric disorders (4, 5)

The σ_1_ receptor subtypes appear to play in a role in motor functions and potassium channels (2). The σ_2_ receptor subtypes are implicated in CNS disorders and malignant neoplastic diseases. Because of these effects, sigma receptor ligands may be useful for the detection and treatment in neurology and oncology. Matsuno et al. (6) developed a potent σ_1_ agonist, 1-(3,4-dimethoxyphenethyl)-4-(3-phenylpropyl)-piperazine dihydrochloride (SA4503), which is in Phase II clinical trials as a therapeutic for functional recovery after stroke. SA4503 is highly selective for σ_1_ receptors than for σ_2_ receptors (6). Small modifications in the SA4503 structure appear to have profound effects on the σ_1_/σ_2_ receptor affinity and selectivity (1). SA5403 has been labeled with ^11^C for PET studies of sigma receptors in monkeys and humans (7-9). However, the equilibrium state of the receptor-ligand binding in monkeys was not possible to measure with [^11^C]SA4503 because of the short t_½_ of ^11^C. In an effort to overcome this problem, Elsinga et al. (1) synthesized [^18^F]FE-SA4503 with a longer physical t_½_ so that the equilibrium state of receptor-ligand binding can be studied.

## Synthesis

[PubMed]

Fujumura et al. (10) reported the synthesis of SA4503 and other analogs of lefetamine. SA4503 was obtained by reacting N,N-bis(2-chloroethyl)-2-(3m4-dimethoxy)phenylethylamine with phenylpropylamine. Elsinga et al. (1) synthesized [^18^F]FE-SA4503 from reacting [^18^F]fluoroethyl tosylate with 1-(4-hydroxy-3-methoxyphenethyl)-4-(3-phenylpropyl)piperazine dichloride (4-O-demethyl SA4503). 4-O-demethyl SA4503 was prepared from the starting material of 3-phenyl-1-propanol (11). [18F]fluoroethyl tosylate was obtained by radiofluorination of the ditosylate precursor at 125 ºC for 5 min. After purification, [^18^F]fluoroethyl tosylate in N,N-dimethylformamide was added to 4-O-demethyl SA4503 and sodium hydride. The reaction mixture was heated at 125 ºC for 5 min. The final product was purified by C_18_-Seppak column and high performance liquid chromatography (HPLC). The radiochemical yield was 4-7% at the end of bombardment with a total synthesis time of 80 min. Using similar synthetic steps, Kawamura et al. (11) modified a FDG-module to an automatic synthesis module for the synthesis of [^18^F]FE-SA4503. The radiochemical yield was 4.4 ± 2.6% (n = 24) with >99% radiochemical purity. The synthesis time was 80 min with a specific activity of at least >100 TBq(2,702 Ci)/mmol at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed]

Elsinga et al. (1) determined that the octanol/water (0.1 M phosphate buffer) coefficient (logP) of [^18^F]FE-SA4503 was 2.66. In comparison, SA4503 had a logP value of 2.52. The in vitro affinity of unlabeled FE-SA4503 was measured by guinea pig brain membranes, and the IC_50_s were reported to be 6.48 nM and 2.11 nM for the σ_1_ and σ_2_ receptors, respectively.

Lever et al. (2) studied the receptor binding affinity of both SA4503 and FE-SA4503 by guinea pig brain membranes. A panel of sigma receptor ligands, haloperidol, (+)-pentazocine, 1,3-di(2-tolyl)guanidine, and ifenprodil, were used to validate the results. FE-SA4503 was 14-fold more selective for σ_1_ (K_i_ = 8.0 nM) over σ_2_ (K_i_ = 113.2 nM) in the guinea pig brain homogenates. In comparison, SA4503 was also14-fold selective for σ_1_ (K_i_ = 4.6 nM) over σ_2_ (K_i_ = 63.1 nM).

## Animal Studies

### Rodents

[PubMed]

Biodistribution of [^18^F]FE-SA4503 was performed in mice with an i.v. dose of 0.2 MBq (5 μCi) (1). The lung and kidney showed a high initial radioactivity localization followed by a rapid decrease. The brain radioactivity concentrations (percent injected dose per g (% ID/g); n = 4) were 4.99 ± 0.45, 4.52 ± 0.18, 3.20 ± 0.18, 2.01 ± 0.13, and 1.23 ± 0.05 at 5, 15, 30, 60, and 120 min, respectively. Blocking studies with haloperidol (a σ_1_ and σ_2_ receptor ligand), SA4503, and (+)-pentazocine (σ_1_ receptor ligand) showed that the brain radioactivity was significantly decreased by pretreatment or co-injection of these ligands. The decrease was observed mainly in cerebellum and cortical regions.

Ex-vivo autoradiography of [^18^F]FE-SA4503 in rats performed by Elsinga et al. (1) showed that the brain distribution was similar to that reported for [^11^C]SA4503 by Kawamura, et al. (8). Hippocampal structures, thalamus, cortical areas, vestibular nucleus, and inferior colliculus were all visible in the axial or coronal cross-sections. Co-injection with SA4503 decreased radioactivity localization in all brain regions. Similar to the reported reduction of [^11^C]SA4503 (8), approximately 80% of the radioactivity was reduced in the regions with high and moderate levels and 70% reduction in the regions with relatively low radioactivity level.

Metabolite studies in rats reported that polar metabolites of [^18^F]FE-SA4503 were present in the plasma, but little was detected in the brain after 30 min of injection (1). About 48.7± 9.5% and 93.4 ± 2.6% (n = 3) of the intact radioligand remained in the plasma and brain tissue, respectively.

### Other Non-Primate Mammals

[PubMed]

No publication is currently available.

### Non-Human Primates

[PubMed]

Elsinga et al. (1) studied the kinetics of [^18^F]FE-SA4503 in a conscious monkey with PET imaging. The monkey received an i.v. dose of 62 MBq (1.7 mCi) of [^18^F]FE-SA4503. PET imaging on the same monkey was also performed with [^11^C]SA4503 (537 MBq(14.5 mCi)) on the next day. The brain distribution of [^18^F]FE-SA4503 was similar to that of [^11^C]SA4503 but the time-activity curve was different. In a study of 6 monkeys, Elsinga et al. (12) injected an i.v. dose of 220-802 MBq (5.5-21.7 mCi) ^18^F]FE-SA4503 with a specific activity >500 GBq(13.5 Ci)/μmol into each monkey. The radioactivity was widely distributed throughout the conscious monkey brain in the PET images at 46-61 min. The radioactivity levels were relatively high in the cortical region, striatum, hippocampus, vermis, and thalamus. In response to treatment with haloperidol (1 mg/kg) or SA4503 (1 mg/kg) at 120 min after ^18^F]FE-SA4503 administration, all radioactivity levels were decreased. A larger reduction in radioactivity uptake was observed with haloperidol pretreatment (30 min before ^18^F]FE-SA4503 injection). Except hippocampus and cerebellum, the time-activity curves were similar in all investigated brain regions. The radioactivity levels increased for the first 15 min, and then there was a gradual decrease. The radioactivity level in the hippocampus increased for 30 min, remained constant for 80 min, and then the level gradually decreased. The radioactivity level in the cerebellum was relatively low. In the metabolite analysis study, 55 ± 24% and 23 ± 10% of ^18^F]FE-SA4503 in the plasma remained unchanged at 30 and 120 min after injection, respectively. Kinetic analysis showed values of binding potentials (association rate constant/dissociation rate constant; k_3_/k_4_) in these areas were1.65-4.04 with the highest value in the hippocampus. The authors suggested that [^18^F]FE-SA4503 was mainly bound to the CNS σ_1_ receptors in vivo.

## Human Studies

[PubMed]

No publication is currently available.

## References

1 Elsinga P.H., Kawamura K., Kobayashi T., Tsukada H., Senda M., Vaalburg W., Ishiwata K. (2002). Synthesis and evaluation of [18F]fluoroethyl SA4503 as a PET ligand for the sigma receptor. Synapse.
2 Lever J.R., Gustafson J.L., Xu R., Allmon R.L., Lever S.Z. (2006). Sigma1 and sigma2 receptor binding affinity and selectivity of SA4503 and fluoroethyl SA4503. Synapse.
3 Skuza G., Wedzony K. (2004). Behavioral pharmacology of sigma-ligands. Pharmacopsychiatry.
4 Skuza G., Rogoz Z. (2002). A potential antidepressant activity of SA4503, a selective sigma 1 receptor agonist. Behav Pharmacol.
5 Ishiguro H., Ohtsuki T., Toru M., Itokawa M., Aoki J., Shibuya H., Kurumaji A., Okubo Y., Iwawaki A., Ota K., Shimizu H., Hamaguchi H., Arinami T. (1998). Association between polymorphisms in the type 1 sigma receptor gene and schizophrenia. Neurosci Lett.
6 Matsuno K., Nakazawa M., Okamoto K., Kawashima Y., Mita S. (1996). Binding properties of SA4503, a novel and selective sigma 1 receptor agonist. Eur J Pharmacol.
7 Kawamura K., Kubota K., Kobayashi T., Elsinga P., Ono M., Maeda M., Ishiwata K. (2005). Evaluation of [11C]SA5845 and [11C]SA4503 for imaging of sigma receptors in tumors by animal PET. Ann Nucl Med.
8 Kawamura K., Ishiwata K., Tajima H., Ishii S., Matsuno K., Homma Y., Senda M. (2000). In vivo evaluation of [(11)C]SA4503 as a PET ligand for mapping CNS sigma(1) receptors. Nucl Med Biol.
9 van Waarde A., Buursma A., Hospers G., Kawamura K., Kobayashi T., Ishii K., Oda K., Ishiwata K., Vaalburg W., Elsinga P. (2004). Tumor imaging with 2 sigma-receptor ligands, 18F-FE-SA5845 and 11C-SA4503: a feasibility study. J Nucl Med.
10 Fujimura K., Matsumoto J., Niwa M., Kobayashi T., Kawashima Y., In Y., Ishida T. (1997). Synthesis, structure and quantitative structure-activity relationships of sigma receptor ligands, 1-[2-(3,4-dimethoxyphenyl)ethyl]-4-(3-phenylpropyl) piperazines. Bioorg Med Chem.
11 Kawamura K., Elsinga P., Kobayashi T., Ishii S., Wang W., Matsuno K., Vaalburg W., Ishiwata K. (2003). Synthesis and evaluation of 11C- and 18F-labeled 1-[2-(4-alkoxy-3-methoxyphenyl)ethyl]-4-(3-phenylpropyl)piperazines as sigma receptor ligands for positron emission tomography studies. Nucl Med Biol.
12 Elsinga P., Tsukada H., Harada N., Kakiuchi T., Kawamura K., Vaalburg W., Kimura Y., Kobayashi T., Ishiwata K. (2004). Evaluation of [18F]fluorinated sigma receptor ligands in the conscious monkey brain. Synapse.